# ^177^Lu-Labeled ethylenediamine tetramethylene phosphonic acid

Chemical name: | ^177^Lu-Labeled ethylenediamine tetramethylene phosphonic acid
Abbreviated name: | [^177^Lu]-EDTMP
Synonym: | (ethylenedinitrilo)-tetramethylenephosphonic acid
Agent Category: | Compound
Target: | Bone (hydroxyapatite) at low concentration; farnesyl disphosphate (pyrophosphate) synthase (molecular target) at high concentration
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure of EDTMP for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=bone%20pain%20palliation&cmd=DetailsSearch)]

Most patients with malignancies of the breast, prostate, lungs, thyroid, or kidneys suffer from severe bone pain due to metastases of the cancer to the skeletal tissue (2, 3). Although several interventions such as analgesics, bisphosphonates, hormone therapy, and systemic radionuclide therapy are available to manage the pain, these treatments are known to have many undesirable secondary effects on the patient (3). Radiopharmaceuticals containing nuclides such as strontium-89 (as ^89^SrCl_2_) and samarium-153 (administered as ^153^Sm-labeled ethylenediamine tetramethylene phosphonic acid (EDTMP)), which have been approved by the United States Food and Drug Administration for the treatment of bone pain due to metastases, are commonly used for palliative care (http://www.who.int/cancer/palliative/definition/en/) of pain in the bones of cancer patients (3). However, these are not ideal agents to treat bone pain because the radionuclide either has a long half-life and generates high-energy β^–^ particles (^89^Sr has a half-life of ~50 days; E_β(max)_ = 1.49 MeV) or is short-lived and has to be produced in close vicinity to the treatment center (^153^Sm has a half-life of ~47 h; E_β(max)_ = 0.81 MeV; Eγ = 103 keV (28%)) (2). A major limitation of using these bone pain palliative agents is that they produce myelotoxicity in some patients (4). Between the two labeled compounds, ^89^SrCl_2_ appears to be the agent of choice for clinical applications because its longer half-life allows some flexibility to develop a suitable treatment regimen for the patient. There is great interest in the development of alternative radiolabeled compounds that can be used to treat pain resulting from osseous metastases (3). An important characteristic of this labeled compound is that it must have the ability to be targeted specifically to the cancerous lesions on the skeleton and should be minimally toxic to the bone marrow as discussed elsewhere (4-6).

In an earlier study with healthy rats, it was reported that EDTMP labeled with lutetium-177 ([^177^Lu]-EDTMP) was cleared rapidly from blood circulation, showed little uptake in the soft tissues, and accumulated primarily in the bones of these animals (7). Chakraborty et al. made similar observations when they investigated the biodistribution of [^177^Lu]-EDTMP in rats (8). A freeze-dried kit for the preparation of [^177^Lu]-EDTMP was developed subsequently by Garnuszek et al. (9). On the basis of these observations, there is a renewed interest to use ^177^Lu (half-life, ~7 days; E_β(max)_ = 497 keV; Eγ = 113 keV (6.4%); 208 keV (11%)) as an alternative nuclide to those currently in use (^89^Sr and ^153^Sm) in the development of a palliative care agent for pain due to the metastases of cancer to the skeletal tissue (5, 6). The main advantages of using ^177^Lu are that it can be easily transported to places where it is not available and the low-energy gamma photons emitted by the nuclide allow detection of the bone lesions with scintigraphy. The biodistribution of [^177^Lu]-EDTMP was studied recently in mice, rats, and rabbits, and scintigraphic imaging was performed on rodents, rabbits, and dogs (5, 6). In addition, the International Atomic Energy Agency has initiated projects to develop ^177^Lu-labeled compounds as palliative care agents for bone pain (6).

### Other Sources of Information

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Phosphonates+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

FDA-approved clinical trials with EDTMP (http://clinicaltrials.gov/ct2/results?term=EDTMP), ^89^SrCl_2_ (http://clinicaltrials.gov/ct2/results?term=Strontium+chloride), and ^153^Sm (http://clinicaltrials.gov/ct2/results?term=Sm-153) complexes

Clinical trials with other-bone imaging agents (http://clinicaltrials.gov/ct2/results?term=Bone+imaging)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase (also known as geranylgeranyl diphosphate synthase 1)

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629)

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Other publications regarding EDTMP in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EDTMP)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-EDTMP%20synthesis&cmd=DetailsSearch)]

The synthesis of [^177^Lu]-EDTMP has been described by Chakraborty et al. (5, 8). The radiochemical yield and purity of the labeled compound were reported to be >98% and >99.0%, respectively, as determined with paper chromatography (R_f_ of [^177^Lu]-EDTMP was ~1, whereas ^177^LuCl_3_, the labeling agent, stayed at the origin) and paper electrophoresis (only [^177^Lu]-EDTMP moved toward the anode). The specific activity of the radiochemical was not reported.

The development of a freeze-dried kit containing sodium EDTMP, stannous chloride, and ascorbic acid for the preparation of [^177^Lu]-EDTMP was reported by Garnuszek et al. (9). The yield of the final labeled product prepared from this kit was >99% as determined with paper chromatography and paper electrophoresis. The specific activity of the radiolabeled compound varied from 3.2 GBq/mg (86 mCi/mg) to 390 GBq/mg (10.5 Ci/mg) depending on the specific activity of the ^177^LuCl_3_ used to prepare the tracer.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-EDTMP%20in%20vitro&cmd=DetailsSearch)]

The [^177^Lu]-EDTMP complex was reported to retain its stability at room temperature for at least 14 days (8). Investigators have also reported that [^177^Lu]-EDTMP prepared from a freeze-dried kit had a purity of >99% over a period of 10 days (9). Chakraborty et al. reported that [^177^Lu]-EDTMP maintained a purity of >99% at room temperature for at least 30 days under in vitro conditions (5). In another study, incubation of [^177^Lu]-EDTMP in the presence of 0.1 M hydrochloric acid was shown to reduce its purity to <70% within 24 h (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-EDTMP%20rodentia&cmd=DetailsSearch)]

In a biodistribution study with normal rats (n = 3–5 animals/time point), radioactivity from [^177^Lu]-EDTMP was reported to clear rapidly from blood circulation and selectively accumulate in the skeletal tissue of the animals (7). This observation was confirmed by several investigators (2, 5, 8-10). In all these studies, only small amounts of radioactivity were detected in the soft tissue of the animals. In addition, a similar biodistribution pattern was observed in rats injected with other ^177^Lu-labeled phosphonates (diethylenetriamine pentamethylene phosphonate, triethylene tetraamine hexamethylene phosphonate, and 1,4,7,10-azacyclododecane-1,4,7,10-tetramethylene phosphonic acid) (8, 10).

Single-photon emission computed tomography (SPECT) imaging of rats injected with [^177^Lu]-EDTMP showed that the tracer was clearly present in all bones and that greater amounts of the label were visible in bones undergoing remodeling (e.g., the back bone and the knee joints of the animals) (10). Similar observations were reported by Mathe et al. (6).

Approximately 41% of the injected radioactivity from [^177^Lu]-EDTMP was shown to accumulate in the bones of mice (n = 5 animals/time point) at 2 h postinjection (p.i.) (6). In this study, little radioactivity was found in soft tissues of the animals compared to the bones. In another study, mice (n = 3 animals) were injected with [^177^Lu]-EDTMP through the tail vein, euthanized 3 days later, and frozen in liquid nitrogen (6). Whole-body autoradiography of cryostat sagittal sections prepared from the frozen animals showed that radioactivity was present primarily on the surface and remodeling areas of the bone. Negligible uptake of the label was observed in the internal spongiosa areas of the skeletal tissue.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-EDTMP%20Non-Primate%20Mammals&cmd=DetailsSearch)]

The biodistribution of [^177^Lu]-EDTMP was investigated in healthy white New Zealand rabbits (n = 3–5 animals/time point) after an injection of the tracer through the ear vein (6, 10). Accumulation of the radiochemical was observed primarily in the bones of the animals, and only small amounts of radioactivity were detected in other tissues, similar to observations from the studies with the mice and rats (see above). Scintigraphy of rabbits injected with [^177^Lu]-EDTMP showed that uptake of the tracer in the skeleton was apparent within 1 h p.i., and the complete skeleton was visible by 3 h p.i (5). Radioactivity in the bones of the rabbits was reported to remain visible for at least 4 weeks p.i (6).

Healthy Beagle dogs were injected intravenously with [^177^Lu]-EDTMP, and whole-body SPECT imaging from 30 min up to 28 days p.i. showed that the label was visible in the skeleton within 3 h p.i., and no accumulation of radioactivity was observed in other major organs or tissues of the animals (5). Similar results were reported by Mathe et al., who performed SPECT imaging studies with Beagle dogs (6).

On the basis of the results presented above, [^177^Lu]-EDTMP can be considered a suitable tracer for the possible initiation of a multicenter human clinical trial coordinated by the International Atomic Energy Agency (6).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-EDTMP%20Non-human%20primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-EDTMP%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Slavicek J.M., Hayes-Plazolles N. (2003). The Lymantria dispar nucleopolyhedrovirus contains the capsid-associated p24 protein gene. Virus Genes.
2 Das T., et al. (2009). (170)Tm-EDTMP: a potential cost-effective alternative to (89)SrCl(2) for bone pain palliation. Nucl Med Biol.
3 Paes F.M., Serafini A.N. (2010). Systemic metabolic radiopharmaceutical therapy in the treatment of metastatic bone pain. Semin Nucl Med.
4 Jansen D.R., et al. (2010). Targeted radiotherapy of bone malignancies. Curr Drug Discov Technol.
5 Chakraborty S., et al. (2008). 177Lu-EDTMP: a viable bone pain palliative in skeletal metastasis. Cancer Biother Radiopharm.
6 Mathe D., et al. (2010). Multispecies animal investigation on biodistribution, pharmacokinetics and toxicity of 177Lu-EDTMP, a potential bone pain palliation agent. Nucl Med Biol.
7 Ando A., et al. (1998). 177Lu-EDTMP: a potential therapeutic bone agent. Nucl Med Commun.
8 Chakraborty S., et al. (2002). 177Lu labelled polyaminophosphonates as potential agents for bone pain palliation. Nucl Med Commun.
9 Garnuszek P., et al. (2003). Evaluation of a freeze-dried kit for EDTMP-based bone-seeking radiopharmaceuticals. Appl Radiat Isot.
10 Chakraborty S., et al. (2008). Comparative studies of 177Lu-EDTMP and 177Lu-DOTMP as potential agents for palliative radiotherapy of bone metastasis. Appl Radiat Isot.